# Cetuximab-Oregon Green 488

Chemical name: | Cetuximab-Oregon Green 488
Abbreviated name: | Cetuximab-OG
Synonym:
Agent Category: | Monoclonal antibody
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor-antibody binding
Method of detection: | Fluorescent imaging
Source of signal: | Oregon Green 488
Activation: | Not required
Studies: | - In vitro; - Rodents | Structure of Cetuximab-OG

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=cetuximab+og)]

The epidermal growth factor receptor (EGFR) is a 170-kDa transmembrane protein that promotes cell proliferation by the specific binding of the autocrine epidermal growth factor (EGF) and transforming growth factor α (TGFα). The activity of these factors is believed to contribute to the progression of cancers. The EGFR operates through a receptor-associated tyrosine kinase–mediated signal transduction pathway that triggers cell proliferation. Overexpression of the EGFR is a characteristic feature of a variety of cancers such as squamous cell lung carcinoma and breast, ovarian, head and neck, bladder, and colon cancers (1). Much evidence indicates, in addition to overexpression, that a mutated EGFR gene may also play a role in development of these cancers (2). The most common mutation results in the development of a truncated receptor gene (EGFRvIII) that is deficient in exons 2–7 of the coding sequence. The mutant gene produces a receptor that lacks a part of the extracellular ligand-binding domain that is not activated by ligand binding. However, the intracellular tyrosine kinase portion of the receptor is active constitutively and autophosphorylates the tyrosine residue that initiates the signaling pathway for cell proliferation. In an effort to develop cancer therapies, a variety of EGFR inhibitors have been developed that either inhibit activation of the receptor kinase or the receptor binding of EGF and TGFα, e.g., monoclonal antibodies (MAb) to the receptor (3, 4).

Cetuximab is a human chimeric anti-EGFR MAb that has been successfully used by itself and in combination with chemo- and radiation therapy for the treatment of solid tumors or metastasized cancers (5, 6). Cetuximab is available commercially in the United States and has been approved (http://www.cancer.gov/cancertopics/druginfo/cetuximab) by the US Food and Drug Administration for the treatment of metastasized colorectal cancer and advanced squamous cell carcinoma of the head and neck. Currently it is being evaluated in several clinical trials (http://www.cancer.gov/search/ResultsClinicalTrialsAdvanced.aspx?protocolsearchid=2740900) for the treatment of a variety of cancers. Because of EGFR heterogeneity in cancers, the imaging of cetuximab binding could assist in the selection and treatment of patients who are likely to respond to treatment and enhance the possibility of a positive outcome of the therapy. Radiolabeled cetuximab has been used to visualize and monitor EGFR tumors in animals and humans (7-10). In an effort to develop a non-radiolabeled imaging agent for EGFR, Aerts et al. developed a fluorescent dye, Oregon Green 488 (OG), and labeled cetuximab with this dye (cetuximab-OG) for the in vitro and in vivo visualization of EGFR in tumor tissue (11).

## Synthesis

[PubMed] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=og+cetuximab+synthesis)

The synthesis of cetuximab-OG was described by Aerts et al. (11). Cetuximab was purchased commercially as a solution and dialyzed against Hepes-buffered saline (pH 7.4). The protein concentration of the dialysate was determined, and the solution was incubated with succinimidyl-acetylacetate to obtain cetuximab-(Lysine)-acetylthioacetate (cetuximab-(Lys)-ATA). The duration of this incubation and yield of the product was not mentioned in the publication. For de-acetylation, cetuximab-(Lys)-ATA was treated with hydroxylamine and ethylenediamine tetraacetic acid (pH 7.4) for 1 h to obtain cetuximab-(Lys)-SH (yield not provided in the publication). This compound was incubated with OG 488–maleimide for 2 h, which resulted in 1:1 labeling (on average) of cetuximab with OG 488. All intermediates and the final product generated by the synthesis were analyzed by matrix-assisted laser desorption/ionization time-of-flight mass spectroscopy. The final yield of cetuximab-OG was not provided in the publication.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=og+cetuximab+in+vitro)]

In vitro binding of cetuximab-OG was investigated in A431 (http://www.biotech.ist.unige.it/cldb/cl160.html) (of human squamous cell carcinoma origin) and T47D (http://www.biotech.ist.unige.it/cldb/cl4454.html) (of human breast tumor origin) cells that have high and low levels of EGFR expression, respectively (11). The cells were incubated with cetuximab-OG for 3 h using an increasing concentration range of the labeled MAb (5.2 fmol to 5.2 µmol). Binding of the labeled MAb was observed under a fluorescent microscope, and only the A431 cells showed clear cetuximab-OG binding with a saturation point of 5.2 nM. The T47D cells had only background levels of cetuximab-OG binding at all concentrations. Subsequently, the T47D cell signals were used as the negative control for all experiments. On average, cetuximab-OG binding in A431 cells was 50-fold higher than the negative controls.

In another study, U-373 cells (http://www.biotech.ist.unige.it/cldb/cl4587.html) (of human glioblastoma-astrocytoma origin) were transfected with a phβAc vector (not described in the publication) containing the EGFRvIII gene (11). A stable clone with the highest expression of EGFRvIII, as determined by immunofluorescence, was selected for further experiments. It was denoted as U373-vIII(+). Another clone that expressed no EGFRvIII was also selected for use as a control and it was denoted as U373-vIII(-). Compared to the U373-vIII(-) cells, the U373-vIII(+) cells had a 40-fold higher binding of cetuximab-OG. This indicated that the labeled MAb could also bind to, and detect, the mutant EGFR.

No competing studies, to determine specificity of the labeled MAb, were reported in the publication (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=og+cetuximab+rodentia)]

The use of cetuximab-OG as an imaging agent was investigated in mice bearing HT-29 cell (http://www.biotech.ist.unige.it/cldb/cl5205.html) tumors (of colorectal origin) (11). Compared to the A431 and the T47D cells, the HT-29 cells express an intermediate level of the EGFR. The labeled MAb was injected into the mice through the tail vein and the animals were euthanized after 5 days. The tumors were excised and prepared for immunohistochemistry. A heterogeneous localization of cetuximab-OG was observed in the tumor sections. EGFR expression was also assessed using a polyclonal antibody against EGFR. The polyclonal antibody also showed a heterogeneous expression pattern of the receptor. Merging images obtained with the two antibodies showed a partial mismatch in cellular accumulation of the two tracers. The extent of mismatch was calculated with a difference map of sections from six representative tumors, where intensity within 20% of the maximum was considered an overlap (a match) and a larger difference was considered a mismatch. This resulted in an overlap of 83.4 ± 5.9%, a mismatch of cetuximab-OG–positive/EGFR-negative of 7.9 ± 5.3%, and a mismatch of cetuximab-OG–negative/EGFR-positive of 8.7 ± 2.1%. According to the investigators, poor vasculature along with perfusion of the tumor, dynamic tumor growth, and necrosis may have limited the uptake of cetuximab-OG. This could have contributed to the in vivo mismatch observed with the two antibodies. The investigators concluded that cetuximab-OG is a promising imaging agent that could be used to visualize both EGFR and EGFRvIII. However, it was indicated for an in vivo study, a mismatch between cell expression of EGFR and cetuximab uptake can be expected.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OG+cetuximab+non+primate+mammals)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OG+cetuximab+non+human+primates)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OG+cetuximab+humans)]

No publications are currently available.

## References

1 Gullick W.J. (1991). Prevalence of aberrant expression of the epidermal growth factor receptor in human cancers. Br Med Bull.
2 Sok J.C., Coppelli F.M., Thomas S.M., Lango M.N., Xi S., Hunt J.L., Freilino M.L., Graner M.W., Wikstrand C.J., Bigner D.D., Gooding W.E., Furnari F.B., Grandis J.R. (2006). Mutant epidermal growth factor receptor (EGFRvIII) contributes to head and neck cancer growth and resistance to EGFR targeting. Clin Cancer Res.
3 Dancey J.E. (2003). Recent advances of molecular targeted agents: opportunities for imaging. Cancer Biol Ther.
4 Dancey J.E., Freidlin B. (2003). Targeting epidermal growth factor receptor--are we missing the mark?. Lancet.
5 Bonner J.A., Harari P.M., Giralt J., Azarnia N., Shin D.M., Cohen R.B., Jones C.U., Sur R., Raben D., Jassem J., Ove R., Kies M.S., Baselga J., Youssoufian H., Amellal N., Rowinsky E.K., Ang K.K. (2006). Radiotherapy plus cetuximab for squamous-cell carcinoma of the head and neck. N Engl J Med.
6 Xiong H.Q., Rosenberg A., LoBuglio A., Schmidt W., Wolff R.A., Deutsch J., Needle M., Abbruzzese J.L. (2004). Cetuximab, a monoclonal antibody targeting the epidermal growth factor receptor, in combination with gemcitabine for advanced pancreatic cancer: a multicenter phase II Trial. J Clin Oncol.
7 Cai W., Chen K., He L., Cao Q., Koong A., Chen X. (2007). Quantitative PET of EGFR expression in xenograft-bearing mice using (64)Cu-labeled cetuximab, a chimeric anti-EGFR monoclonal antibody. Eur J Nucl Med Mol Imaging.
8. Pantaleo, M.A., S. Fanti, P.L. Lollini, S. Boschi, and G. Biasco, PET detection of epidermal growth factor receptor in colorectal cancer: a real predictor of response to cetuximab treatment? Eur J Nucl Med Mol Imaging, 2007.
9 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
10 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
11 Aerts H.J., Dubois L., Hackeng T.M., Straathof R., Chiu R.K., Lieuwes N.G., Jutten B., Weppler S.A., Lammering G., Wouters B.G., Lambin P. (2007). Development and evaluation of a cetuximab-based imaging probe to target EGFR and EGFRvIII. Radiother Oncol.